# Anti-vascular endothelial growth factor polylactic acid-polyethylene glycol-poly-L-Lys/gadolinium-diethylenetriamine pentaacetic acid nanoparticles

Chemical name: | Anti-vascular endothelial growth factor polylactic acid-polyethylene glycol-poly-L-Lys/gadolinium-diethylenetriamine pentaacetic acid nanoparticles
Abbreviated name: | Anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs, anti-VEGF PLA-PEG-PLL-Gd NPs
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor (VEGF)
Target category: | Protein
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium (Gd)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T1 relaxation and lead to brighter contrast images.

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (2). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (3). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (2).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (4). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (5, 6). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (7-9). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease. Therefore, it is important to measure VEGF levels in the tumors for designing better anti-cancer treatment protocols. Bevacizumab is a humanized antibody against VEGF-A. It binds to all VEGF isoforms. Bevacizumab is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer. Nagengast et al. (10) prepared ^89^Zr-N-succinyldesferrioxamine-bevacizumab (^89^Zr-bevacizumab) for imaging VEGF expression in nude mice bearing SKOV-3 human ovarian tumor xenografts.

VEGF has been demonstrated to be overexpressed in hepatocellular carcinoma (HCC) compared with normal tissue, even in early stages of HCC (11). Liu et al. (12) used polylactic acid-polyethylene glycol-poly-L-Lys as a multifunctional encapsulating agent composed of gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA) and anti-VEGF monoclonal antibody (anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs) for use in MRI to target VEGF expression in HCC.

### Related Resource Links:

- Chapters in MICAD (VEGF (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGF+antibody+AND+micad%5Bbook%5D))
- Gene information in NCBI (VEGF (http://www.ncbi.nlm.nih.gov/gene/7422))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGF (http://omim.org/entry/192240))
- Clinical trials (VEGF (http://www.clinicaltrials.gov/ct2/results?term=VEGF), Bevacizumab (http://www.clinicaltrials.gov/ct2/results?term=Bevacizumab), Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA))
- FDA Drug information (VEGF (http://google2.fda.gov/search?q=anti-VEGF&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), Bevacizumab (http://google2.fda.gov/search?q=Bevacizumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20synthesis)]

PLA-PEG-PLL-DTPA-Gd NPs were prepared with a solvent diffusion method as described by Liu et al. (12). A mixture of PLA-PEG-PLL-DTPA (40 mg) and PLA-PEG-PLL (20 mg) was dissolved in 2 mL dimethylformamide (DMF). The organic polymer solution was added into 40 mL aqueous solution at 12 mL/h at room temperature and stirred for 2 h. DMF was removed by dialyzed against deionized water for 72 h. PLA-PEG-PLL-DTPA-Gd NPs were concentrated by centrifugation. Anti-VEGF monoclonal antibody (clone not specified) was linked on the glutaraldehyde-activated amino group of PLL on the surface of PLA-PEG-PLL-DTPA-Gd NPs after incubation for 12 h at 4°C. Anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs were washed three times to removed unbound antibody. For flow cytometry studies, fluorescein-labeled NPs (PLA-PEG-PLL-FITC NPs and anti-VEGF PLA-PEG-PLL-FITC NPs) were also prepared. The average numbers of PLA-PEG and PLA-PEG-PLL groups per NP were 9,500 and 12,800, respectively. The mean diameters of PLA-PEG-PLL-DTPA-Gd NPs, anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs, and anti-VEGF PLA-PEG-PLL-FITC NPs (n = 3/group) as determined with photon correlation spectroscopy were 69.8 ± 5.3 nm, 85.8 ± 7.2 nm, and 85.2 ± 5.8 nm, respectively. The larger diameters of anti-VEGF NPs indicate that the antibody is successfully linked to the NPs. The zeta potential values for PLA-PEG-PLL-DTPA-Gd NPs, anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs, and anti-VEGF PLA-PEG-PLL-FITC NPs were 23.03 ± 4.6 mv, 21.63 ± 2.4 mv, and 22.77 ± 2.5 mv, respectively. The similar zeta potential values of the three NPs suggest that the antibody linkage has little effect on their surface charge. No aggregation of these NPs was observed with transmission electronic microscopy in blood plasma after up to 4 h of incubation. The number of antibody moieties and Gd^3+^ ions per NP were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20in%20vitro)]

T1- and T2-Weighted MRI of anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs (Gd = 0.6–12.0 µM) and DTPA-Gd ([Gd] = 40 µM) were performed at 3.0 T at room temperature (12). For T1-weighted imaging, the signal of 8 µM anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs was similar to that of 40 µM DTPA-Gd. The r_1_ and r_2_ relaxivity values of anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs were 18.39 mM^–1^s^–1^ and 24.86 mM^–1^s^–1^, respectively.

Human HCC HepG2 cells exhibited dose- and time-dependent accumulation of anti-VEGF PLA-PEG-PLL-FITC NPs (0.25–0.75 mg/ml NPs) at 37°C as determined with flow cytometry analysis, whereas PLA-PEG-PLL-FITC NPs showed only minimal accumulation (12). DTPA-Gd, PLA-PEG-PLL-DTPA-Gd NPs, anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs, and anti-VEGF PLA-PEG-PLL-FITC showed no cytotoxic effect at 40 µM for 24 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20rodentia)]

Liu et al. (12) performed quantitative T1 MRI at 3.0 T in mice bearing mouse hepatocarcinoma HC22 xenografts at various time points after intravenous injection of 40 µmol/kg DTPA-Gd, PLA-PEG-PLL-DTPA-Gd NPs, or anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs. DTPA-Gd distributed all over the body shortly after injection and returned to normal at 1 h after injection. The signal intensity reached the maximum in the tumor at 10 min and then declined rapidly. The maximum signal intensity of the kidney was higher than those of the tumor, liver, heart, and muscle at 10 min and declined relatively slowly. PLA-PEG-PLL-DTPA-Gd NPs showed a slight signal enhancement in the tumor at 1 h and reached a maximum at 3 h. The tumor boundary was clearly visualized. This represents non-specific binding. The signal intensity of the heart reached a maximum at ~1 min and declined slowly. At 12 h, the signal intensities of the tumor and normal tissues all returned to the background levels. Anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs showed maximum signal intensity in the tumor at 2 h and declined slowly. The tumor signal intensity was still visualized at 12 h and returned to background level at 24 h. The signal intensities of the heart, liver, and muscle showed similar enhancement curves compared with PLA-PEG-PLL-DTPA-Gd NPs. Both NPs showed significant target enhancements to the tumor, liver, heart, and muscle compared with DTPA-Gd (P < 0.01). Anti-VEGF PLA-PEG-PLL-DTPA-Gd NPs showed significantly higher tumor enhancement (P < 0.01) compared with PLA-PEG-PLL-DTPA-Gd NPs, which in turn showed significantly higher tumor enhancement (P < 0.01) compared with DTPA-Gd. Blocking studies were not performed with the anti-VEGF antibody, though DTPA-Gd and PLA-PEG-PLL-DTPA-Gd NPs were used as controls.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Anti-VEGF%20PLA%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
3 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
4 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
5 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
6 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
7 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
9 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
10 Nagengast W.B., de Vries E.G., Hospers G.A., Mulder N.H., de Jong J.R., Hollema H., Brouwers A.H., van Dongen G.A., Perk L.R., Lub-de Hooge M.N. (2007). In vivo VEGF imaging with radiolabeled bevacizumab in a human ovarian tumor xenograft. J Nucl Med.
11 Finn R.S., Zhu A.X. (2009). Targeting angiogenesis in hepatocellular carcinoma: focus on VEGF and bevacizumab. Expert Rev Anticancer Ther.
12 Liu Y., Chen Z., Liu C., Yu D., Lu Z., Zhang N. (2011). Gadolinium-loaded polymeric nanoparticles modified with Anti-VEGF as multifunctional MRI contrast agents for the diagnosis of liver cancer. Biomaterials.